# (-)-4-[^11^C]Methoxycarbonyl-2-[(1-pyrrolidinylmethyl]-1-[(3,4-dichlorophenyl)acetyl]-piperidine

Chemical name: | (-)-4-[^11^C]Methoxycarbonyl-2-[(1-pyrrolidinylmethyl]-1-[(3,4-dichlorophenyl)acetyl]-piperidine
Abbreviated name: | [^11^C]GR103545, (-)-[^11^C]GR89696
Synonym:
Agent category: | Compound
Target: | Kappa opioid (κ) receptor
Target category: | Receptor
Method of detection: | Positron emission tomography (PET)
Source of signal: | ^11^C
Activation: | No
Studies: | - In vitro; - Rodents; - Non-human Primates | Click on the above structure for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=11C%20GR103545)]

Opioids such as morphine are commonly used analgesics in clinical practice. Three opioid receptors (mu, µ; delta, δ; and kappa, κ) that mediate opioid effects have been identified by molecular cloning: δ (enkephalin-preferring), κ (dynorphin-preferring), and µ (ß-endorphin-preferring) (1). Each type of opioid receptors consists of subtypes of receptors as suggested by pharmacological studies (2, 3). Their specificity and ubiquitous location are present in both the central and peripheral nervous system. The opioid receptors (G-protein coupled, resulting in decrease in adenylyl cyclase activity) play an important role in the regulation of analgesia, shock, appetite, thermoregulation, cardiovascular, mental and endocrine function (2-5). Although µ opioid receptors are the major receptor to mediate the analgesic effects of opioids, δ and κ receptors are also important in antinociception. Opioids have been found to protect cells from ischemia injury in the heart and brain via the δ receptors. On the other hand, κ antagonist prevents neurodegeneration.

In humans, the κ opioid receptors (κ_1_ and κ_2_ ) are the most abundant brain opioid receptors and are widely distributed in deeper layers of the neocortex (particularly temporal, parietal, and frontal cortices), striatum, and thalamus, with lower levels in the amygdala, hippocampus, occipital cortex, and cerebellum (6, 7). The κ opioid receptors have been implicated in several clinical brain disorders, including substance abuse (8), epilepsy (9), Tourette’s syndrome (10), and Alzheimer’s disease (11).

(±)-4-Methoxycarbonyl-2-[(1-pyrrolidinylmethyl]-1-[(3,4-dichlorophenyl)acetyl]-piperidine (GR89696) is a novel, highly potent, and selective κ opioid receptors agonist (12). The (–)-isomer, (–)-4-methoxycarbonyl-2-[(1-pyrrolidinylmethyl]-1-[(3,4-dichlorophenyl)acetyl]-piperidine, also known as GR103545, is the more potent optical isomer of GR89696 (IC_50_, 0.018 nM versus 6.0 nM). GR89696 is centrally penetrating, with a log P value of 3.14, and has potent antinociceptive, sedative, and diuretic effects. K_i_ values for GR89696 κ_1_- and κ_2_-receptor binding are in the low nanomolar or subnanomolar range. GR89,696 is an agonist for κ_2_ opioid receptors and an antagonist at κ_1_ receptors in the guinea pig hippocampus (13). [^11^C]GR103545 is being developed as a PET agent for the non-invasive study of the κ receptors in the brain.

### Related Resource Links:

- Chapters in MICAD (Kappa opioid (κ) receptor (http://www.ncbi.nlm.nih.gov/books?term=Kappa%20opioid%20receptor%20AND%20micad%5Bbook%5D))
- Gene information in NCBI (Kappa opioid (κ) receptor (http://www.ncbi.nlm.nih.gov/gene/4986))
- Articles in Online Mendelian Inheritance in Man (OMIM) (Kappa opioid (κ) receptor (http://omim.org/entry/165196))
- Clinical trials (Kappa opioid (κ) receptor (http://www.clinicaltrials.gov/ct2/results?term=Kappa+opioid+AND+receptor))
- Drug information in FDA (Kappa opioid (κ) receptor (http://google2.fda.gov/search?q=kappa+opioid+receptor&client=FDAgov&site=FDAgov&lr=&proxystylesheet=FDAgov&output=xml_no_dtd&getfields=*))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=11C%20GR103545%20and%20synthesis)]

Ravert et al. (14) reported synthesis of [^11^C]GR89696 by N-acetylation of the corresponding normethylcarbamoyl precursor ((±)-1-[(3,4-dichlorophenyl)acetyl]-4-(phenylmethyl)-2-[(1-pyrrolidinyl)methyl]piperidine) with [^11^C]methyl chloroformate in the presence of triethylamine in ethylene chloride. An average radiochemical yield was 20% with a total synthesis time of 29 min. An average specific activity was 75.5 GBq/μmol (2794 mCi/μmol at end of synthesis) with a radiochemical purity of >99%. Later, the same procedure was used to prepared the (+)- and (-)- [^11^C]enantiomer using the (+)- or (-)- normethylcarbamoyl precursor with the average yields of 14% and specific activities of 69.3 MBq/nmol (2.6 mCi/nmol at end of synthesis) (15). Chemical purity was >95% and radiochemical purity was >98%.

Nabulsi et al. (16) reported a two-step, one-pot procedure of [^11^C]GR103545 in an automated synthesis. In the first step, the normethylcarbamoyl precursor was converted to the carbamic acid intermediate desmethyl-GR103545 via transcarboxylation with the zwitterionic carbamic complex, 1,8-diazabicyclo[5.4.0]undec-7-ene-carbon dioxide in the presence and of cesium carbonate and tetrabutylammonium triflate. In the second step, the intermediate was radiolabeled at the carboxyl oxygen with [^11^C]methyl trifluoromethanesulfonate to provide [^11^C]GR103545 with >94% radiochemical purity and a specific activity of 322 ± 81 MBq/nmol (8.7 ± 2.2 mCi/nmol) at the end of synthesis (n = 15). The radiochemical yield was 8.2 ± 2.5% with the total synthesis time of ~43 min.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=11C%20GR103545%20and%20in%20vitro)]

Naylor et al. (17) reported in vitro functional assays using rabbit vas deferens (κ-specific tissue, IC_50_ = 0.041 nM), rat vas deferens (µ -specific tissue, IC_50_ > 10,000 nM), and hamster vas deferens (δ -specific tissue IC_50_ > 10,000 nM). As reported by Butelman et al. (18), GR89696 displaced [^3^H]bremazocine binding (representing both κ_1_- and κ_2_-receptors) with a K_i_ of 1.15 ± 0.47 nM in the rhesus monkey cortical membranes. K_i_ values for the κ_1_- and κ_2_-receptors were 0.5 and 6.3 nM, respectively. GR89696 also displaced binding of [^3^H]DAMGO ([D-Ala (2),N-Me-Phe (4),Gly-ol(5)]-enkephalin, µ-sites) and [^3^H]DPDPE ([D-Pen2,5]-enkephalin, δ-sites) with K_i_ values of 0.65 ± 0.15 and 30.61 ± 11.8 nM, respectively. GR89696 was a potent, high-efficacy agonist on cloned κ-receptors expressed in CHO cells, as measured by its ability to stimulate [^35^S]GTPγS binding (ED_50_, 0.097 ± 0.005 nM), whereas GR89696 was approximately 100-fold less potent at µ-receptors in C6 glioma cells (ED_50_, 9.5 ± 2.4 nM).

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=11C%20GR103545%20and%20rodentia)]

Ex vivo biodistribution studies in CD-1 mice injected with 7-15 MBq (0.2-0.4 mCi, 3 μg/kg) were performed by Ravert et al. (14) showing high accumulation of radioactivity in the brain (5.4% injected dose (ID) at 5 min post injection). The cerebellum radioactivity was washed out most rapidly with a half-life of 16 min. Brain region to cerebellum ratios increased over time with ratios at 90 min of 7.8, 5.6, and 4.5 for the hypothalamus, olfactory tubercle, and striatum, respectively. The accumulation of [^11^C]GR89696 correlated with known κ opioid receptor densities and was inhibited by κ_1_ opioid agonist (U69593) and GR89696 but not by 5HT-2 antagonist (ketanserin) and D_2_ antagonist (spiperone).

[^11^C]GR103545 (the (-)-enantiomer of [^11^C]GR89696), demonstrated high affinity in mouse brain with hypothalamus/cerebellum and olfactory tubercle/cerebellum ratios of 11.4 and 8.7 at 90 minutes (15), respectively. (+)-[^11^C]GR89696 showed low affinity and region-to-cerebellum ratios of 1 for all brain regions. The accumulation of [^11^C]GR103545 in the olfactory tubercle, hypothalamus, striatum and pre-frontal cortex was inhibited by pretreatment with GR103545 with 50% at 0.01 mg/kg and 85-96% at 0.1 mg/kg, whereas GR89696 was less potent with <10% inhibition at 0.01 mg/kg and 40-62% at 0.2mg/kg. Pretreatment with naltrindole (δ) and cyprodime (µ) showed no effect on the binding of [^11^C]GR103545 in these brain areas. [^11^C]GR103545 exhibited a selective and saturable binding for the κ opioid receptor.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=11C%20GR103545%20%28dog%20or%20pig%20or%20sheep%20or%20rabbit%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=11C%20GR103545%20%28primate%20not%20human%29)]

Talbot et al. (19) studied three adult male baboons with [^11^C]GR103545 and [^11^C]GR89696 PET imaging under baseline conditions and after pretreatment with an opioid receptor competitive antagonist, naloxone (1 mg/kg). Regional total distribution volume [V_T_] values and specific-to-nonspecific equilibrium partition coefficients (V_3_”) were derived using the arterial input function and a 2-tissue-compartment model. High levels of [^11^C]GR103545 radioactivity were found in cingulate cortex (V_T_ = 10.91 ± 6.1 ml/g), striatum (V_T_ = 10.5 ± 5.9 ml/g), frontal cortex (V_T_ = 8.5 ± 3.7 ml/g), temporal cortex (V_T_ = 8.1 ± 4.3 ml/g), and parietal cortex (V_T_ = 7.5 ± 3.8 ml/g). Intermediate levels were found in thalamus (V_T_ = 6.9 ± 3.6 ml/g) and medial temporal lobe (V_T_ = 7.0 ± 3.8 ml/g), and low levels in brain stem (V_T_ = 5.1 ± 2.9 ml/g) and occipital cortex (V_T_ = 4.9 ± 2.5 ml/g). Lowest levels were found in the cerebellum (V_T_ = 3.7 ± 1.6 ml/g). Pretreatment with naloxone revealed that the specific binding of [^11^C]GR103545 in all regions were reduced to low levels (V_3_” = 0.1-0.4), whereas little effect was found in the cerebellum. V_3_” values of [^11^C]GR103545 in all regions (cerebellum as a reference) were higher than [^11^C]GR89696, whereas (+)-[^11^C]GR89696 V_3_” values were negligible. The fraction of unchanged [^11^C]GR103545 in plasma samples determined by HPLC was 27% at 60 min after injection.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=11C%20GR103545%20and%20human)]

No publication is currently available.

## NIH Support

R21 DA66505-01, K012 MH01603-01

## References

1 Minami M., Satoh M. (1995). Molecular biology of the opioid receptors: structures, functions and distributions. Neurosci Res.
2 Satoh M., Minami M. (1995). Molecular pharmacology of the opioid receptors. Pharmacol Ther.
3 Waldhoer M., Bartlett S.E., Whistler J.L. (2004). Opioid receptors. Annu Rev Biochem.
4 Molina P.E. (2006). Opioids and opiates: analgesia with cardiovascular, haemodynamic and immune implications in critical illness. J Intern Med.
5 Barry U., Zuo Z. (2005). Opioids: old drugs for potential new applications. Curr Pharm Des.
6 Hiller J.M., Fan L.Q. (1996). Laminar distribution of the multiple opioid receptors in the human cerebral cortex. Neurochem Res.
7 Peckys D., Landwehrmeyer G.B. (1999). Expression of mu, kappa, and delta opioid receptor messenger RNA in the human CNS: a 33P in situ hybridization study. Neuroscience.
8 Mello N.K., Negus S.S. (2000). Interactions between kappa opioid agonists and cocaine. Preclinical studies. Ann N Y Acad Sci.
9 de Lanerolle N.C., Williamson A., Meredith C., Kim J.H., Tabuteau H., Spencer D.D., Brines M.L. (1997). Dynorphin and the kappa 1 ligand [3H]U69,593 binding in the human epileptogenic hippocampus. Epilepsy Res.
10 Chappell P.B., Leckman J.F., Scahill L.D., Hardin M.T., Anderson G., Cohen D.J. (1993). Neuroendocrine and behavioral effects of the selective kappa agonist spiradoline in Tourette's syndrome: a pilot study. Psychiatry Res.
11 Mathieu-Kia A.M., Fan L.Q., Kreek M.J., Simon E.J., Hiller J.M. (2001). Mu-, delta- and kappa-opioid receptor populations are differentially altered in distinct areas of postmortem brains of Alzheimer's disease patients. Brain Res.
12 Birch P.J., Rogers H., Hayes A.G., Hayward N.J., Tyers M.B., Scopes D.I., Naylor A., Judd D.B. (1991). Neuroprotective actions of GR89696, a highly potent and selective kappa-opioid receptor agonist. Br J Pharmacol.
13 Caudle R.M., Mannes A.J., Iadarola M.J. (1997). GR89,696 is a kappa-2 opioid receptor agonist and a kappa-1 opioid receptor antagonist in the guinea pig hippocampus. J Pharmacol Exp Ther.
14 Ravert H.T., Mathews W.B., Musachio J.L., Scheffel U., Finley P., Dannals R.F. (1999). [11C]-methyl 4-[(3,4-dichlorophenyl)acetyl]-3-[(1-pyrrolidinyl)-methyl]-1- piperazinecarboxylate ([11C]GR89696): synthesis and in vivo binding to kappa opiate receptors. Nucl Med Biol.
15 Ravert H.T., Scheffel U., Mathews W.B., Musachio J.L., Dannals R.F. (2002). [(11)C]-GR89696, a potent kappa opiate receptor radioligand; in vivo binding of the R and S enantiomers. Nucl Med Biol.
16 Nabulsi N.B., Zheng M.Q., Ropchan J., Labaree D., Ding Y.S., Blumberg L., Huang Y. (2011). [11C]GR103545: novel one-pot radiosynthesis with high specific activity. Nucl Med Biol.
17 Naylor A., Judd D.B., Lloyd J.E., Scopes D.I., Hayes A.G., Birch P.J. (1993). A potent new class of kappa-receptor agonist: 4-substituted 1-(arylacetyl)-2-[(dialkylamino)methyl]piperazines. J Med Chem.
18 Butelman E.R., Ko M.C., Traynor J.R., Vivian J.A., Kreek M.J., Woods J.H. (2001). GR89,696: a potent kappa-opioid agonist with subtype selectivity in rhesus monkeys. J Pharmacol Exp Ther.
19 Talbot P.S., Narendran R., Butelman E.R., Huang Y., Ngo K., Slifstein M., Martinez D., Laruelle M., Hwang D.R. (2005). 11C-GR103545, a radiotracer for imaging kappa-opioid receptors in vivo with PET: synthesis and evaluation in baboons. J Nucl Med.